# N-4-Fluorobut-2-yn-1-yl-2β-carbo-[^11^C]methoxy-3β-phenyltropane

Chemical name: | N-4-Fluorobut-2-yn-1-yl-2β-carbo-[^11^C]methoxy-3β-phenyltropane
Abbreviated name: | [^11^C]PR04.MZ
Synonym:
Agent category: | Compound
Target: | Dopamine transporter (DAT)
Target category: | Transporter
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PR04.MZ)]

Dopamine, a neurotransmitter, plays an important role in the mediation of movement, cognition, and emotion. Parkinson’s disease (PD) is associated with a loss of dopamine-containing neurons in the striatum, resulting in a loss of dopamine transporter (DAT) in the presynaptic nerve terminals (1, 2). Reduction of DAT density is inversely correlated with the severity of motor dysfunction in PD patients. Several (-)-cocaine analogs were developed for the evaluation of DAT density in neurons of PD patients. Radiolabeled 2β-carboxymethoxy-3β-(4-iodophenyl)tropane (β-CIT) and N-(3-fluoropropyl)-2β-carbomethoxy-3β-(4-iodophenyl)nortropane (FP-CIT) have been used for brain imaging (3-6). Because of the short physical half-life of ^11^C-labeled analogs, equilibrium conditions are difficult to achieve in positron emission tomography (PET) measurements. [^123^I]β-CIT was studied in single-photon emission computed tomography (SPECT) and showed slow tracer uptake kinetics (7, 8). A tropane derivative, [^11^C]-(E)-N-(4-fluorobut-2-enyl)-2β-carbomethoxy-3β-(4'-tolyl)nortropane ([^11^C]LBT-999), was evaluated as a radioligand for studies of DAT with PET imaging (9-11). N-4-Fluorobut-2-yn-1-yl-2β-carbo-[^11^C]methoxy-3β-phenyltropane ([^11^C]PR04.MZ) was developed through the use of a conformational restriction approach based on (-)-cocaine (12). PR04.MZ exhibited a 100-fold higher potency than (-)-cocaine in inhibition of human DAT and better selectivity over the human noradrenalin transporter (hNET) and human serotonin transporter (hSERT). [^11^C]PR04.MZ has been evaluated as a radioligand for studies of DAT with PET imaging.

### Related Resource Links:

- Chapters in MICAD (DAT (http://www.ncbi.nlm.nih.gov/books?term=(DAT%20or%20dopamine%20transporter)%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (DAT (http://www.ncbi.nlm.nih.gov/gene/6531))
- Articles in Online Mendelian Inheritance in Man (OMIM) (DAT (http://www.ncbi.nlm.nih.gov/omim/126455))
- Clinical trials (DAT (http://www.clinicaltrials.gov/ct2/results?term=DAT+imaging))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PR04.MZ%20AND%20synthesis)]

[^11^C]PR04.MZ was synthesized with a standard methylation reaction of its corresponding O-desmethyl trifluoroacetic acid salt precursor with [^11^C]methyl iodide and rubidium carbonate in N,N-dimethylformamide (75°C, 5 min) (12). The radiochemical yields (non-decay corrected) were >20% (n = 3). The radiochemical purity was >98%, with a specific activity of 67 GBq/µmol (1.8 Ci/µmol) at the end of synthesis. The total synthesis time was 45 min.

## In Vitro studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PR04.MZ%20AND%20in%20vitro)]

PR04.MZ binding affinity for hDAT, hSERT, and hNET was determined using stably transfected HEK293 cells (12). [^3^H]β-CFT, [^3^H]citalopram, and [^3^H]nisoxetine were used as radioligands, respectively. The 50% inhibition concentration values for hDAT, hSERT, and hNET were 1.9 ± 0.2 nM, 108.4 ± 1.3 nM, and 22.5 ± 0.8 nM, respectively.

## Animal Studies

### Rodents

[PubMed] (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PR04.MZ%20AND%20rodentia)

Riss et al. (12) performed dynamic PET brain scans in one normal rat for 60 min as a preliminary study after injection of 37 MBq (1 mCi) [^11^C]PR04.MZ. The peak striatal accumulation of 2.22% injected dose per cm^3^ of tissue was reached at 4 min after injection, and this accumulation decreased only slightly for the duration of the scans. The striatum/cerebellum ratios were 2.4, 3.6, and 5.0 at 15, 30, and 60 min after injection. Pretreatment (45 min before [^11^C]PR04.MZ injection) with GBR12909, a structurally unrelated DAT inhibitor, decreased the striatum/cerebellum ratio to 1.6 at 60 min after injection.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=PR04.MZ+AND+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PR04.MZ%20AND%20monkeys)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PR04.MZ%20AND%20human)]

No publication is currently available.

## References

1 Carbon M., Ghilardi M.F., Feigin A., Fukuda M., Silvestri G., Mentis M.J., Ghez C., Moeller J.R., Eidelberg D. (2003). Learning networks in health and Parkinson's disease: reproducibility and treatment effects. Hum Brain Mapp.
2 Chesselet M.F., Delfs J.M. (1996). Basal ganglia and movement disorders: an update. Trends Neurosci.
3 Abi-Dargham A., Gandelman M.S., DeErausquin G.A., Zea-Ponce Y., Zoghbi S.S., Baldwin R.M., Laruelle M., Charney D.S., Hoffer P.B., Neumeyer J.L., Innis R.B. (1996). SPECT imaging of dopamine transporters in human brain with iodine-123-fluoroalkyl analogs of beta-CIT. J Nucl Med.
4 Chaly T., Dhawan V., Kazumata K., Antonini A., Margouleff C., Dahl J.R., Belakhlef A., Margouleff D., Yee A., Wang S., Tamagnan G., Neumeyer J.L., Eidelberg D. (1996). Radiosynthesis of [18F] N-3-fluoropropyl-2-beta-carbomethoxy-3-beta-(4-iodophenyl) nortropane and the first human study with positron emission tomography. Nucl Med Biol.
5 Kazumata K., Dhawan V., Chaly T., Antonini A., Margouleff C., Belakhlef A., Neumeyer J., Eidelberg D. (1998). Dopamine transporter imaging with fluorine-18-FPCIT and PET. J Nucl Med.
6 Lundkvist C., Halldin C., Ginovart N., Swahn C.G., Farde L. (1997). [18F] beta-CIT-FP is superior to [11C] beta-CIT-FP for quantitation of the dopamine transporter. Nucl Med Biol.
7 Ishikawa T., Dhawan V., Kazumata K., Chaly T., Mandel F., Neumeyer J., Margouleff C., Babchyck B., Zanzi I., Eidelberg D. (1996). Comparative nigrostriatal dopaminergic imaging with iodine-123-beta CIT-FP/SPECT and fluorine-18-FDOPA/PET. J Nucl Med.
8 Laruelle M., Wallace E., Seibyl J.P., Baldwin R.M., Zea-Ponce Y., Zoghbi S.S., Neumeyer J.L., Charney D.S., Hoffer P.B., Innis R.B. (1994). Graphical, kinetic, and equilibrium analyses of in vivo [123I] beta-CIT binding to dopamine transporters in healthy human subjects. J Cereb Blood Flow Metab.
9 Chalon S., Hall H., Saba W., Garreau L., Dolle F., Halldin C., Emond P., Bottlaender M., Deloye J.B., Helfenbein J., Madelmont J.C., Bodard S., Mincheva Z., Besnard J.C., Guilloteau D. (2006). Pharmacological characterization of (E)-N-(4-fluorobut-2-enyl)-2beta-carbomethoxy-3beta-(4'-tolyl)nortropane (LBT-999) as a highly promising fluorinated ligand for the dopamine transporter. J Pharmacol Exp Ther.
10 Dolle F., Emond P., Mavel S., Demphel S., Hinnen F., Mincheva Z., Saba W., Valette H., Chalon S., Halldin C., Helfenbein J., Legaillard J., Madelmont J.C., Deloye J.B., Bottlaender M., Guilloteau D. (2006). Synthesis, radiosynthesis and in vivo preliminary evaluation of [11C]LBT-999, a selective radioligand for the visualisation of the dopamine transporter with PET. Bioorg Med Chem.
11 Saba W., Valette H., Schollhorn-Peyronneau M.A., Coulon C., Ottaviani M., Chalon S., Dolle F., Emond P., Halldin C., Helfenbein J., Madelmont J.C., Deloye J.B., Guilloteau D., Bottlaender M. (2007). [11C]LBT-999: a suitable radioligand for investigation of extra-striatal dopamine transporter with PET. Synapse.
12 Riss P.J., Hooker J.M., Alexoff D., Kim S.W., Fowler J.S., Rosch F. (2009). [(11)C]PR04.MZ, a promising DAT ligand for low concentration imaging: Synthesis, efficient (11)C-O-methylation and initial small animal PET studies. Bioorg Med Chem Lett.